# ^68^Ga-1,4,7,10-Tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid-Lys^40^-exendin-3

Chemical name: | ^68^Ga-1,4,7,10-Tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid-Lys^40^-exendin-3
Abbreviated name: | ^68^Ga-DOTA-Lys^40^-exendin-3
Synonym:
Agent category: | Peptide
Target: | Glucagon-like peptide-1 receptor (GLP-1R)
Target category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^68^Ga
Activation: | No
Studies: | - In vitro; - Rodents | Structure not available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=68Ga%20Exendin-3)]

Glucagon-like peptide-1 (GLP-1, 30 amino acids) is secreted from enteroendocrine cells of the distal small intestine in response to food ingestion (1). GLP-1 plays an important role in glucose metabolism and homeostasis, and it inhibits gastric emptying, glucagon secretion, and glucose production (2). In addition, GLP-1 induces insulin release from β-cells in the pancreas. GLP-1 also induced proliferation of the pancreatic β-cells. The GLP-1 receptor (GLP-1R) has been identified in normal tissues such as the pancreas, stomach, brain, and lung, and it has been shown to be highly overexpressed in human insulinomas and gastrinomas (3). In insulinomas, GLP-1R density is considerably greater, and the GLP-1R is more frequently observed than somatostatin receptors.

Exendin-4 is a GLP-1 analog with 39 amino acids isolated from the venom of the Gila monster (Heloderma suspectum) (4). Exendin-4 and GLP-1 share a 53% amino acid sequence homology. Exendin-4 is a more potent and longer-lasting GLP-1R agonist than GLP-1. Exendin-4 is resistant to cleavage by dipeptidyl peptidase IV, whereas the first two N-terminal amino acids of GLP-1 are rapidly cleaved. ^111^In-Diethylenetriamine pentaacetic acid-aminohexanoic acid-Lys^40^-exendin-4 (^111^In-DTPA-Ahx-Lys^40^-exendin-4) has been developed for single-photon emission computed tomography (SPECT) imaging of the GLP-1R (5, 6). Exendin-3 and exendin-4 differ in two amino acids (positions 2 and 3), which are located in the region of the peptide that is responsible for internalization of the ligand-receptor complex. Brom et al. (7) investigated the usefulness of ^68^Ga-1,4,7,10-tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid-Lys^40^-exendin-3 (^68^Ga-DOTA-Lys^40^-exendin-3) as a positron emission tomography (PET) agent for imaging insulinomas.

### Related Resource Links:

- Chapters in MICAD (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=GLP-1%5BAll+Fields%5D+AND+micad%5Bbook%5D)
- Gene information in NCBI (GLP-1R (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=gene&Cmd=DetailsSearch&Term=2740%5Buid%5D)).
- Articles in OMIM (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=omim&Cmd=DetailsSearch&Term=GLP-1)
- Clinical trials (Exendin (http://www.clinicaltrials.gov/ct2/results?term=GLP-1))
- Drug information in FDA (http://google2.fda.gov/search?q=exendin&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=11&y=18)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=68Ga%20Exendin-3%20and%20synthesis)]

A mixture of 185 MBq (5 mCi) ^68^Ga and DOTA-Lys^40^-exendin-3 was incubated in buffer (pH 3.0) for 15 min at 95°C (7). ^68^Ga-DOTA-Lys^40^-exendin-3 was identified with high-performance liquid chromatography (HPLC). ^68^Ga-DOTA-Lys^40^-exendin-3 exhibited a radiochemical purity of >99% and a specific activity of 110 GBq/µmol (3 Ci/µmol) after HPLC purification.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=68Ga%20Exendin-3%20and%20in%20vitro)]

Brom et al. (7) reported that ^nat^In-DTPA-Lys^40^-exendin-3, ^nat^In-DOTA-Lys^40^-exendin-3, and ^nat^Ga-DOTA-Lys^40^-exendin-3 exhibited 50% inhibitory concentration (IC_50_) values of 8.5 nM, 5.3 nM, and 5.7 nM, respectively. The inhibition assays were performed with GLP-1R–expressing rat insulinoma INS-1 cells and ^111^In-DTPA-Lys^40^-exendin-3.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=68Ga%20Exendin-3%20and%20rodentia)]

Brom et al. (7) performed biodistribution studies in nude mice (n = 5) bearing INS-1 insulinomas that consisted of injection of 1 MBq (37 μCi) ^68^Ga-DOTA-Lys^40^-exendin-3. An experiment that consisted of coinjection of excess exendin-3 was also performed. Tumor accumulation was 8.9 ± 3.1% injected dose/gram (ID/g) at 1 h after injection. Excess exendin-3 reduced the tumor accumulation to the background level (~1% ID/g). Specific and moderate uptake was observed in the pancreas, stomach, lung, and duodenum. Uptake in the kidneys was ~120% ID/g and was not displaced by exendin-3. Marginal accumulation (<1% ID/g) was observed in the muscle, blood, heart, spleen, and liver. As a comparison, tumor accumulation of ^68^Ga-DOTA-Lys^40^-exendin-3 was approximately two-fold lower than that of ^111^In-DTPA-Lys^40^-exendin-3 and ^111^In-DTPA-Lys^40^-exendin-4.

^68^Ga-DOTA-Lys^40^-exendin-3 PET imaging in mice identified high uptake in the kidneys and tumor at 1 h after injection. No blocking studies were performed in the PET experiments.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=68Ga%20Exendin-3%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=68Ga%20Exendin-3%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=68Ga%20Exendin-3%20and%20human)]

No publication is currently available.

## NIH Support

1R01 AG030328-01

## References

1 Theodorakis M.J., Carlson O., Michopoulos S., Doyle M.E., Juhaszova M., Petraki K., Egan J.M. (2006). Human duodenal enteroendocrine cells: source of both incretin peptides, GLP-1 and GIP. Am J Physiol Endocrinol Metab.
2 Doyle M.E., Egan J.M. (2001). Glucagon-like peptide-1. Recent Prog Horm Res.
3 Reubi J.C., Waser B. (2003). Concomitant expression of several peptide receptors in neuroendocrine tumours: molecular basis for in vivo multireceptor tumour targeting. Eur J Nucl Med Mol Imaging.
4 Meier J.J., Nauck M.A. (2005). Glucagon-like peptide 1(GLP-1) in biology and pathology. Diabetes Metab Res Rev.
5 Gotthardt M., Lalyko G., van Eerd-Vismale J., Keil B., Schurrat T., Hower M., Laverman P., Behr T.M., Boerman O.C., Goke B., Behe M. (2006). A new technique for in vivo imaging of specific GLP-1 binding sites: First results in small rodents. Regul Pept.
6 Wild D., Behe M., Wicki A., Storch D., Waser B., Gotthardt M., Keil B., Christofori G., Reubi J.C., Macke H.R. (2006). [Lys40(Ahx-DTPA-111In)NH2]Exendin-4, a Very Promising Ligand for Glucagon-like Peptide-1 (GLP-1) Receptor Targeting. J Nucl Med.
7 Brom M., Oyen W.J., Joosten L., Gotthardt M., Boerman O.C. (2010). 68Ga-labelled exendin-3, a new agent for the detection of insulinomas with PET. Eur J Nucl Med Mol Imaging.